# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-panitumumab

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane- N,N',N'',N'''-tetraacetic acid- panitumumab
Abbreviated name: | ^64^Cu-DOTA-Panitumumab
Synonym:
Agent category: | Chimeric monoclonal antibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20panitumumab)]

Epidermal growth factor (EGF) is a 53-amino-acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab (a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody against the extracellular domain of recombinant HER2) (11) was labeled as ^111^In-trastuzumab (12-14). C225 (an anti-EGFR, mouse-human chimeric, monoclonal IgG_1_ antibody, also known as cetuximab) was labeled as ^99m^Tc-EC-C225 (15, 16) for single-photon emission computed tomography (SPECT) imaging of EGFR expression on solid tumors. However, positron emission tomography (PET) offers better sensitivity, resolution, and quantification than SPECT (17). ^64^Cu (t_1/2_ = 12.7 h, β^-^ decay) is an attractive radionuclide for labeling cetuximab. Panitimumab has been approved by the United States Food and Drug Administration as a single agent for the treatment of EGFR-expressing, metastatic colorectal carcinoma. For evaluation as a PET imaging agent, ^64^Cu was attached to panitumumab via 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to form ^64^Cu-DOTA-panitumumab. Niu et al. (18) performed PET imaging studies in nude mice bearing human head and neck squamous cell carcinoma (HNSCC) tumors with different expressions of EGFR and found an unexpected inverse relationship with radioactivity accumulation and EGFR density in the tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550)
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab), panitumumab (http://www.clinicaltrials.gov/ct2/results?term=panitumumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18), panitumumab (http://google2.fda.gov/search?q=panitumumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=15&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20panitumumab%20and%20synthesis)]

Monofunctional N-hydroxysuccinimide ester and 1-ethyl-3-[3-(dimethylamino)-propyl] carbodiimide (EDC) were used to activate DOTA to conjugate panitumumab to form DOTA-panitumumab, which was purified with column chromatography (18). DOTA per antibody was determined to be ~20. ^64^CuCl_2_ was added to DOTA-panitumumab. The reaction mixture was incubated for 60 min at 40°C. ^64^Cu-DOTA-panitumumab was purified with column chromatography. The yield of ^64^Cu-DOTA-cetuximab was 85.0 ± 9.2% with specific activities of 20 MBq/nmol (0.54 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20panitumumab%20and%20in%20vitro)]

Niu et al. (18) performed cell-binding assays with panitumumab using EGFR-expressing HNSCC 22B, SAS, and SQB20 cell lines. FITC-Conjugated donkey anti-IgG was used as a secondary antibody for detection with flow cytometry. The fluorescence intensity was 300, 900, and 4,000 for 22B, SAS, and SQB20, respectively. Tumor sections from these cell lines showed that SQB20 (high fluorescence intensity) had the highest EGFR expression, followed by SAS (moderate fluorescence intensity) and 22B (low fluorescence intensity).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20panitumumab%20and%20rodentia)]

Niu et al. (18) studied the whole-body distribution of ^64^Cu-DOTA-panitumumab (7–8 MBq/mouse or 0.19–0.22 mCi/mouse) with the use of PET imaging (static scans at 4, 20, 30, and 48 h) in 22B (low EGFR-expression), SAS (moderate EGFR-expression), and SQB20 (high EGFR-expression) xenograft tumors in mice (n = 4). Tumor accumulation of ^64^Cu-DOTA-panitumumab was highest in 22B tumors at all time points; tumor accumulation was lowest in SQB20 tumors. At 30 h, the 22B, SAS, and SQB20 tumor accumulation levels were 31.4% injected dose/gram (ID/g), 12.4% ID/g, and 8.7% ID/g, respectively. Radioactivity accumulation remained high in the liver (12.0% ID/g) and blood (12.4% ID/g) but was low in the muscle (2.8% ID/g). No blocking experiment was performed. However, the tumor-imaging study was also performed with ^64^Cu-DOTA-IgG. Tumor accumulation of ^64^Cu-DOTA-IgG was also higher in 22B tumors at all time points than in SAS and SQB20 tumors. At 30 h, the 22B, SAS, and SQB20 tumor accumulation levels were 11.8% ID/g, 7.2% ID/g, and 7.3% ID/g, respectively. Accumulation of ^64^Cu-DOTA-IgG in the liver, blood, and muscle was similar to that found with ^64^Cu-DOTA-panitumumab. Immunohistological studies with anti-CD31 (platelet endothelial cell adhesion molecule-1) staining showed that DOTA-panitumumab exhibited the lowest perivascular localization with CD31 in both SQB20 and SAS tumors. Furthermore, the microvascular density of the three tumors as determined with CD31 showed that 22B tumors (27.1/mm^2^) were highly vascularized as compared with SAS tumors (12.5/mm^2^) and SQB20 tumors (4.7/mm^2^). Evan blue perfusion showed that 22B tumors were more permeable than ASA tumors, which were more permeable than SQB20 tumors. Therefore, the authors concluded that the low microvascular density and poor vascular permeability are likely responsible for the low tumor accumulation of ^64^Cu-DOTA-panitumumab in SQB20 tumors, which express high levels of EGFR.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20panitumumab%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20panitumumab%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20panitumumab%20and%20human)]

No publication is currently available.

## NIH Support

P50 CA114747, R21 CA102123, R24 CA93862, U54 CA119367, R01 CA118582

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
16 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
17 Lundqvist H., Tolmachev V. (2002). Targeting peptides and positron emission tomography. Biopolymers.
18 Niu G., Li Z., Xie J., Le Q.T., Chen X. (2009). PET of EGFR antibody distribution in head and neck squamous cell carcinoma models. J Nucl Med.